# ^125^I-Labeled monoclonal antibody PSA30

Chemical name: | ^125^I-Labeled monoclonal antibody PSA30
Abbreviated name: | ^125^I-PSA30
Synonym:
Agent Category: | Antibodies
Target: | free, unbound form (fPSA) of prostate-specific antigen (PSA)
Target Category: | Antigens
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PSA%20and%20imaging%20and%20antibody%20and%20prostate%20cancer)]

^125^I-Labeled monoclonal antibody (mAb) PSA30, abbreviated as ^125^I-PSA30, was developed by Evans-Axelsson et al. for use in prostate cancer imaging by targeting the free, unbound form (fPSA) of prostate-specific antigen (PSA) (1).

The human kallikrein-related peptidases (KLKs) are a group of 15 secreted serine proteases with different expression patterns and physiological roles (2, 3). These KLKs exist as single-chain preproenzymes of 30–40 kDa and are overproduced in various malignancies, where they are involved in diverse cancer-related processes such as cell growth regulation, angiogenesis, invasion, and metastasis (2, 4). Several members of the KLKs have been shown to be useful as prognostic biomarkers in various malignancies, with PSA being the most widely accepted and broadly used in clinical practice (4).

PSA is encoded by the KLK3 gene and produced in abundance at almost all clinical stages and grades of prostate cancer (1, 2). An important finding is that, after synthesis in the cells, PSA is then released into the blood and exists in a noncatalytic form by forming stable covalent complexes (cPSA) with extracellular protease inhibitors, particularly a-1-antichymotrypsin (ACT) (5, 6). A smaller percentage (5%–40%) of the noncatalytic PSA in the blood also presents as a free, unbound form, which is unable to form complexes with inhibitors despite ~10^4^-fold excess presence of inhibitors in the blood (1, 7). Because of its small size (28.4 kDa), fPSA is eliminated via glomerular filtration by the kidneys, with a half-life time of 12–18 h (7). In contrast, cPSA (~90 kDa) is eliminated very slowly, possibly via the liver. Measurements of the serum fPSA and cPSA are used for screening, diagnosis, and prognostic prediction of prostate cancer as well as for monitoring cancer recurrence.

Prostate cancer imaging with radiolabeled antibodies by targeting PSA was tested as early as 15–20 years ago (8-10). However, these studies were in general unable to delineate tumors with a good signal/noise ratio because of the high background activity. One reason for the failure might be the use of polyclonal antibodies as imaging agents, which not only cross-react with other antigens but also fail to discriminate fPSA from cPSA. Evans-Axelsson et al. hypothesized that in vivo imaging of prostate cancer, especially the disseminated cancer, might be feasible by targeting the fPSA based on the facts that fPSA, rather than cPSA, is present at high abundance in close proximity to its local site of production, and that fPSA is cleared rapidly from the blood by the kidneys (1). The investigators tested their hypothesis by radiolabeling the PSA30 mAb and imaging tumors in animal models of prostate cancer (1). PSA30 recognizes an epitope that is covered by the ACT and other inhibitors, but is accessible on fPSA (11, 12).

### Related Resource Links:

Articles about KLK3 gene function (http://www.ncbi.nlm.nih.gov/pubmed?term=KLK3%20gene%20function) in PubMed

Human KLK3 gene database (http://www.ncbi.nlm.nih.gov/gene/354)

Prostate cancer clinical trials (http://www.clinicaltrials.gov/ct2/results?term=prostate+cancer&Search=Search) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22489659)]

Evans-Axelsson et al. labeled the PSA30 antibody with ^125^I using the Iodogen method (1). The labeling reaction was carried out for 15 min at room temperature. The radiochemical purity was 95% after gel filtration. Two metabolic probes, 2-^18^F-FDG and ^18^F-choline, were also produced with an in-house cyclotron. The radiochemical purity for both probes was >99%. The radiochemical yield and specific activity were not reported for the three imaging agents.

An immunoradiometric assay was used to estimate the binding quality of ^125^I-PSA30 (1). The estimation showed that ^125^I-PSA30 maintained 87% of the binding affinity of the unlabeled PSA30 antibody. No data for ^125^I-PSA30 binding affinity with either fPSA or cPSA were provided.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22489659)]

No data are available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22489659)]

Biodistribution of ^125^I-PSA30 was studied in non–tumor-bearing mice (n = 14) and LNCaP tumor–bearing nude mice (n = 34) (1). Each mouse was administered ~10 MBq (27 μCi, 15 μg) ^125^I-PSA30 through the tail vein. The radioactive uptake in each organ was presented as decay-corrected percentage of injected activity per gram of tissue (% IA/g).

For studies in non–tumor-bearing mice, organs were collected, and the radioactivity in each organ was measured at 6, 24, 96, 168, and 312 h, respectively, after injection (n = 2–3 mice/group). A decrease of the radioactivity from the first measurement after injection was observed in all tested organs (except for the thyroid) and blood (Table 1). The decrease during the first 24 h ranged from 55% to 83% in the liver, kidney, and blood. The highest uptake was found in organs with high residual blood content. The organ/blood ratios in highly vascularized organs remained largely unchanged over time, which is in accordance with the fact that PSA is not expressed in non-primate species, including mice. The radioactivity in thyroid increased from 6 h to 168 h after injection, indicating dehalogenation.

Table 1: Biodistribution of ^125^I-PSA30 (percent of IA/g) in nontumor-bearing mice.

Tissue | 6 h (n = 3) | 24 h (n = 3) | 96 h (n = 3) | 168 h (n = 2) | 312 h (n = 3)
Blood | 13.12 ± 12.99 | 2.52 ± 2.26 | 3.76 ± 0.56 | 2.27 ± 0.40 | 1.32 ± 0.61
Kidneys | 4.04 ± 3.18 | 0.69 ± 0.63 | 1.04 ± 0.11 | 0.49 ± 0.23 | 0.28 ± 0.16
Liver | 1.64 ± 1.62 | 0.75 ± 0.79 | 0.85 ± 0.08 | 0.48 ± 0.14 | 0.24 ± 0.12
Prostate | 2.34 ± 2.08 | 0.55 ± 0.58 | 0.72 ± 0.16 | 0.66 ± 0.13 | 0.41 ± 0.11
Brain | 0.29 ± 0.22 | 0.07 ± 0.07 | 0.08 ± 0.01 | 0.05 ± 0.01 | 0.03 ± 0.01
Thyroid^a^ | 6.0 ± 5.8 | 14 ± 22 | 26 ± 8.0 | 19 ± 3.0 | 25 ± 5.0

^a^Thyroid data presented as % IA per whole organ.

For studies in LNCaP tumor–bearing nude mice, organs were collected, and the activity in each organ was measured at 4, 24, 72, 168, and 312 h, respectively, after injection (n = 5–8 mice/group). Similar to the findings in non–tumor-bearing mice, highly vascularized organs initially showed high activity levels, which rapidly decreased from the first measurement after injection (Table 2). The organ/blood ratios remained largely unchanged over time in most organs. LNCaP tumors had a higher uptake than most tested organs and peaked (4.32% IA/g) at 24 h, with a subsequent sharp decrease by 72 h after injection (Table 2). In comparison to non–tumor-bearing mice, the radioactive accumulation in thyroid was greatly augmented, and there was a sharp increase at 72 h after injection. This inverse correlation between tumor and thyroid radioactivity was considered to be due to dehalogenation.

Table 2: Biodistribution of ^125^I-PSA30 (percent of IA/g) in LNCaP tumor-bearing mice.

Tissue | 4 h (n = 8) | 24 h (n = 8) | 72 h (n = 8) | 168 h (n = 5) | 312 h (n = 5)
Tumor | 3.27 ± 3.35 | 4.32 ± 5.26 | 1.39 ± 1.26 | 0.56 ± 0.54 | 0.10 ± 0.13
Blood | 7.44 ± 3.86 | 5.56 ± 4.20 | 4.00 ± 2.24 | 1.19 ± 1.57 | 0.46 ± 0.62
Kidneys | 3.12 ± 3.78 | 1.66 ± 1.13 | 1.02 ± 0.67 | 0.39 ± 0.41 | 0.15 ± 0.20
Liver | 1.90 ± 1.19 | 1.66 ± 1.48 | 1.07 ± 0.68 | 0.35 ± 0.34 | 0.10 ± 0.14
Prostate | 1.07 ± 0.50 | 0.97 ± 0.66 | 0.71 ± 0.44 | 0.22 ± 0.28 | 0.14 ± 0.17
Brain | 0.28 ± 0.35 | 0.13 ± 0.11 | 0.09 ± 0.05 | 0.03 ± 0.03 | 0.01 ± 0.02
Thyroid^a^ | 23 ± 21 | 31 ± 22 | 104 ± 64 | 105 ± 48 | 48 ± 23

^a^Thyroid data presented as % IA per whole organ.

The radioactive distribution within tumors was imaged with digital autoradiography of tumor sections. LNCaP tumor–bearing mice (n = 36) were first administered ^125^I-PSA30 (10 MBq, 27 μCi). In two mice, ^18^F-choline was then administered at 48 h after injection of ^125^I-PSA30, and in five mice ^18^F-FDG (n = 5) was administered at 24, 72, 168, and 312 h after injection of ^125^I-PSA30. Animals were euthanized 1 h after injection of the metabolic probes, and tumors were immediately removed and cut into 100-μm sections for imaging or into 20-μm sections for tumor pathology and PSA immunohistochemistry. Differences in both emission spectra and rate of decay were used to generate separate images of each radionuclide in animals injected with more than one radionuclide, in this case, ^125^I and ^18^F. Tumor section images showed uniform distribution of ^125^I-PSA30 in tumor areas containing densely packed viable cells. High activity of ^125^I-PSA30 was manifested in the proximity to blood vessels, capillaries, and areas with viable PSA-secreting tumor cells. Except for areas of necrosis, there was a close similarity between the distribution of PSA revealed by immunohistochemistry and high radioactivity of ^125^I-PSA30 on images, but there was little association between the high activity of ^125^I-PSA30 and the uptake of ^18^F-choline or ^18^F-FDG (1). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Evans-Axelsson S., Ulmert D., Orbom A., Peterson P., Nilsson O., Wennerberg J., Strand J., Wingardh K., Olsson T., Hagman Z., Tolmachev V., Bjartell A., Lilja H., Strand S.E. (2012). Targeting free prostate-specific antigen for in vivo imaging of prostate cancer using a monoclonal antibody specific for unique epitopes accessible on free prostate-specific antigen alone. Cancer Biother Radiopharm.
2 Avgeris M., Mavridis K., Scorilas A. (2010). Kallikrein-related peptidase genes as promising biomarkers for prognosis and monitoring of human malignancies. Biol Chem.
3 Papachristopoulou G., Avgeris M., Charlaftis A., Scorilas A. (2011). Quantitative expression analysis and study of the novel human kallikrein-related peptidase 14 gene (KLK14) in malignant and benign breast tissues. Thromb Haemost.
4 Lilja H., Ulmert D., Vickers A.J. (2008). Prostate-specific antigen and prostate cancer: prediction, detection and monitoring. Nat Rev Cancer.
5 Christensson A., Laurell C.B., Lilja H. (1990). Enzymatic activity of prostate-specific antigen and its reactions with extracellular serine proteinase inhibitors. Eur J Biochem.
6 Lilja H., Christensson A., Dahlen U., Matikainen M.T., Nilsson O., Pettersson K., Lovgren T. (1991). Prostate-specific antigen in serum occurs predominantly in complex with alpha 1-antichymotrypsin. Clin Chem.
7 Bruun L., Savage C., Cronin A.M., Hugosson J., Lilja H., Christensson A. (2009). Increase in percent free prostate-specific antigen in men with chronic kidney disease. Nephrol Dial Transplant.
8 Dillman R.O., Beauregard J., Ryan K.P., Hagan P.L., Clutter M., Amox D., Frincke J.M., Bartholomew R.M., Burnett K.G., David G.S., et al. (1987). Radioimmunodetection of cancer with the use of indium-111-labeled monoclonal antibodies. NCI Monogr.
9 Perala-Heape M., Vihko P., Pelkonen I., Laine A., Vihko R. (1991). Effect of conjugation on the biodistribution of 111In-labelled anti-PAP and anti-PSA monoclonal antibodies examined in nude mice with PC-82 human tumor xenografts. In Vivo.
10 Babaian R.J., Murray J.L., Lamki L.M., Haynie T.P., Hersh E.M., Rosenblum M.G., Glenn H.J., Unger M.W., Carlo D.J., von Eschenbach A.C. (1987). Radioimmunological imaging of metastatic prostatic cancer with 111indium-labeled monoclonal antibody PAY 276. J Urol.
11 Nilsson O., Peter A., Andersson I., Nilsson K., Grundstrom B., Karlsson B. (1997). Antigenic determinants of prostate-specific antigen (PSA) and development of assays specific for different forms of PSA. Br J Cancer.
12 Piironen T., Villoutreix B.O., Becker C., Hollingsworth K., Vihinen M., Bridon D., Qiu X., Rapp J., Dowell B., Lovgren T., Pettersson K., Lilja H. (1998). Determination and analysis of antigenic epitopes of prostate specific antigen (PSA) and human glandular kallikrein 2 (hK2) using synthetic peptides and computer modeling. Protein Sci.